# p-(2-[^18^F]Fluoroethyl)-L-phenylalanine

Chemical name: | p-(2-[^18^F]Fluoroethyl)-L-phenylalanine
Abbreviated name: | [^18^F]FEP
Synonym:
Agent category: | Compound
Target: | L-type amino acid transporter system
Target category: | Transporter
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20fluoroethyl%20phenylalanine)]

A variety of ^11^C- and ^18^F-labeled amino acids have been studied for potential use in positron emission tomography (PET) oncology (1, 2). Most brain tumors show an increased uptake of amino acids compared with uptake in normal brain tissue. These amino acids are composed of naturally occurring amino acids, such as L-[^11^C]leucine, L-[^11^C]methionine (MET), and L-[^11^C]tyrosine, and non-natural amino acids, such as [^11^C]aminoisobutyric acid, [^11^C]1-aminocyclopentane-1-carboxylic acid, and [^11^C]1-aminocyclobutane-1-carboxylic acid. ^123^I-Labeled amino acids are also used for imaging in oncology although no radiolabeled amino acid is approved at present (1, 3, 4).

More than twenty amino acid transporter systems have been identified (1). Most of the amino acids are taken up by tumor cells through an energy-independent L-type amino acid transporter system and a Na-dependent transporter system A, as well as through a Na^+^-dependent system B^0^ (5). The amino acids are retained in tumor cells due to their high metabolic activities, including incorporation into proteins, which are higher than metabolic activities of most normal cells (1). Malignant transformation increases the use of amino acids for energy, protein synthesis, and cell division. Tumor cells were found to have overexpressed transporter systems (6). L-[^11^C]MET, [^18^F]fluorotyrosine, L-[^11^C]leucine, and [^18^F]fluoro-α-methyl tyrosine have been widely used in the detection of tumors (2, 5), but they are not approved by the United States Food and Drug Administration. These radiolabels are moved into cells by various amino acid transporters and are incorporated into proteins although only leucine is quantitatively incorporated into protein. The fraction of radiolabeled amino acids that is incorporated into proteins is usually small compared to the total amount taken up into the cell. Imaging techniques that use natural amino acids are based on amino acid transport and protein incorporation.

Non-natural amino acids are not incorporated into proteins (2, 7); instead, they are rapidly transported into tumor cells. They are retained inside the tumor cells because of their high cellular metabolism and the high activity of the amino acid transporters. A new L-tyrosine analog, O-(2-[^18^F]fluoroethyl)-L-tyrosine ([^18^F]FET), was synthesized and evaluated as an amino acid PET tracer for the detection of brain tumors.[^18^F]FET has a higher specificity than [^18^F]FDG. Recently, a new L-phenylalanine analog, p-(2-[^18^F]fluoroethyl)-L-phenylalanine ([^18^F]FEP), was synthesized and evaluated as an amino acid PET tracer for the detection of brain tumors (8). FEP is a substrate for the L-type amino acid transporter system. Therefore, [^18^F]FEP could be a useful tracer in brain tumor imaging based solely on amino acid transport.

### Related Resource Links:

- Chapters in MICAD (Amino acid transporters (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=amino%20acid%20(transporter%20OR%20transporters)+AND+micad%5Bbook%5D))
- Gene information in NCBI (L-type amino acid transporter (http://www.ncbi.nlm.nih.gov/gene/23428), A-type amino acid transporter (http://www.ncbi.nlm.nih.gov/gene/54407))
- Articles in Online Mendelian Inheritance in Man (OMIM) (Amino acid transporters (http://www.ncbi.nlm.nih.gov/omim?Db=omim&Cmd=DetailsSearch&Term=amino%5BAll+Fields%5D+AND+acid%5BAll+Fields%5D+AND+transporter%5BAll+Fields%5D))
- Clinical trials (Amino acid transporters (http://www.clinicaltrials.gov/ct2/results?term=amino+acid+transporters))
- Drug information in FDA (Amino acid transporters (http://google2.fda.gov/search?q=amino+acid+transporters&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=13&y=15))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20fluoroethyl%20phenylalanine%20and%20synthesis)]

Wang et al. (8) reported the synthesis of [^18^F]FEP using the tosylate precursor in a two-step reaction. Nucleophilic [^18^F]fluorination was performed in the presence of tetra-butyl ammonium bicarbonate, with subsequent acidic hydrolysis to remove the protecting groups. The specific activity of [^18^F]FEP was 31–69 GBq/μmol (0.84–1.84 Ci/μmol) at the end of synthesis, with a total synthesis time of 90 min and a radiochemical decay-corrected yield of 27%–37%. Radiochemical purity was >95%.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20fluoroethyl%20phenylalanine%20and%20in%20vitro)]

Wang et al. (8) showed that [^18^F]FEP entered rat 9L gliosarcoma tumor cells in culture with 13.3% incubation dose/0.1 mg protein (n = 3) after 30 min of incubation. [^18^F]FEP uptake into rat 9L gliosarcoma tumor cells in culture was reduced by 90%, 5%, and 50% by the presence of 1 mM 2-aminobicyclo[2.2.1]heptane-2-carboxylic acid (an L-type transporter inhibitor), N-methyl-α-aminoisobutyric acid (an A-type transporter inhibitor), and serine, respectively. The data suggest that [^18^F]FEP is predominantly transported into 9L cells via the L-type transporter.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20fluoroethyl%20phenylalanine%20and%20rodentia)]

The biodistribution of [^18^F]FEP was studied in 9L glioma-bearing rats (n = 6) (8^8^). Moderate uptake of [^18^F]FEP was observed in most organs, such as kidneys, liver, lung, blood, brain, and heart (0.52%–0.65% ID/g), with the highest uptake in the pancreas (2.45% ID/g) at 60 min after injection. The tumor uptake of [^18^F]FEP was 0.90% ID/g, and accumulation was low in the bone (0.41% ID/g). The tumor/blood and tumor/muscle ratios were 1.73 and 1.45, respectively. PET imaging dynamic scans were performed with [^18^F]FEP in comparison to [^18^F]FET at 5–120 min after injection. Both tracers showed rapid tumor accumulation at 5 min and reached a plateau at ~20 min. The tumor/muscle ratios (~5) of these two tracers were similar at 20 min after injection. No blocking studies were performed.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20fluoroethyl%20phenylalanine%20and%20%28dog%20or%20pig%20or%20rabbit%20or%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20fluoroethyl%20phenylalanine%20l%20tyrosine%20and%20primate%20not%20human)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20fluoroethyl%20phenylalanine%20and%20human)]

No publication is currently available.

## References

1 Jager P.L., Vaalburg W., Pruim J., de Vries E.G., Langen K.J., Piers D.A. (2001). Radiolabeled amino acids: basic aspects and clinical applications in oncology. J Nucl Med.
2 Laverman P., Boerman O.C., Corstens F.H., Oyen W.J. (2002). Fluorinated amino acids for tumour imaging with positron emission tomography. Eur J Nucl Med Mol Imaging.
3 Langen K.J., Pauleit D., Coenen H.H. (2002). 3-[(123)I]Iodo-alpha-methyl-L-tyrosine: uptake mechanisms and clinical applications. Nucl Med Biol.
4 Lahoutte T., Caveliers V., Camargo S.M., Franca R., Ramadan T., Veljkovic E., Mertens J., Bossuyt A., Verrey F. (2004). SPECT and PET amino acid tracer influx via system L (h4F2hc-hLAT1) and its transstimulation. J Nucl Med.
5 Langen K.J., Jarosch M., Muhlensiepen H., Hamacher K., Broer S., Jansen P., Zilles K., Coenen H.H. (2003). Comparison of fluorotyrosines and methionine uptake in F98 rat gliomas. Nucl Med Biol.
6 Saier M.H., Daniels G.A., Boerner P., Lin J. (1988). Neutral amino acid transport systems in animal cells: potential targets of oncogene action and regulators of cellular growth. J Membr Biol.
7 Wester H.J., Herz M., Weber W., Heiss P., Senekowitsch-Schmidtke R., Schwaiger M., Stocklin G. (1999). Synthesis and radiopharmacology of O-(2-[18F]fluoroethyl)-L-tyrosine for tumor imaging. J Nucl Med.
8 Wang L., Qu W., Lieberman B.P., Plossl K., Kung H.F. (2011). Synthesis, uptake mechanism characterization and biological evaluation of (18)F labeled fluoroalkyl phenylalanine analogs as potential PET imaging agents. Nucl Med Biol.